# QD800-Polyethylene glycol-Cys-Z_HER2:342_ Affibody

Chemical name: | QD800-Polyethylene glycol-Cys-Z_HER2:342_ Affibody
Abbreviated name: | QD800-PEG-Z_HER2:342_
Synonym:
Agent category: | Antibody
Target: | Epidermal growth factor receptor (HER2)
Target category: | Receptor
Method of detection: | Optical, near-infrared (NIR) fluorescence imaging
Source of signal: | Quantum dot (QD)
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=54792098), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?val=NM_201282.1) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=Graphics&list_uids=2064) for more information about HER2.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes)]

Epidermal growth factor (EGF) is a 53-amino–acid growth factor (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys, and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF, with at least seven other growth factors and their transmembrane receptor kinases, play important roles in cell proliferation, survival, adhesion, migration, and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3), and HER4 (erbB-4) (2). HER1, HER3, and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain, and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells, such as breast, non-small-cell lung, head and neck, and colon cancers (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor patient prognosis because high levels are related to increased proliferation (7-10).

Fluorescent semiconductor quantum dots (QDs) are nanocrystals made of CdSe/CdTe-ZnS with radii of 1–10 nm (11-13). They can be tuned to emit in a range of wavelengths by changing their sizes and composition, thus providing broad excitation profiles and high absorption coefficients. They have narrow and symmetric emission spectra with long, excited-state lifetimes (20–50 ns), as compared with that of fluorescent dyes (1–10 ns). They possess good quantum yields of 40%–90% and high extinction coefficients. They are more photostable than conventional organic dyes. They can be coated and capped with hydrophilic materials for additional conjugations with biomolecules, such as peptides, antibodies, nucleic acids, and small organic compounds, which were tested in vitro and in vivo (13-17). Although many cells have been labeled with QDs in vitro with little cytotoxicity, there are only limited studies of long-term toxicity of QDs in small animals (18-26). Furthermore, little is known about the toxicity and the mechanisms of clearance and metabolism of QDs in humans. QDs that do not contain Cd (non-Cd QDs) have been prepared as an alternative to the more toxic Cd-based QDs. These newly developed non-Cd QDs exhibit improved blood half-life and minimal reticuloendothelial system accumulation with rapid renal clearance (27). These QDs easily extravasate leaky tumor blood vessels because of the enhanced permeability and retention effect.

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (28). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (29-33). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab')_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on a 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (34). These Affibody molecules exhibit high binding affinity to HER2, with K_d_ values of <50 pM. Various radiolabeled HER2 Affibody molecules have been studied in terms of their ability to image HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. The synthetic Affibody molecule Cys-Z_HER2:342_ Affibody was targeted to HER2 and conjugated to QD800 coated with polyethylene glycol (PEG) to form QD800-PEG-Z_HER2:342_ (35). QD800-PEG-Z_HER2:342_ nanoparticles were evaluated for near-infrared (NIR) fluorescence imaging in nude mice bearing human SKOV3 ovarian carcinoma tumor.

### Related Resource Links:

- Chapters in MICAD (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064))
- Articles in Online Mendelian Inheritance in Man (OMIM) (HER2 (http://omim.org/entry/164870))
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20synthesis)]

QD800 (InAs/InP/ZnSe) nanoparticles (5 nm in diameter) were coated with PEG phosphatidylethanolamine (DSPE-PEG2000 amine) by hydrophobic-hydrophobic interactions (35). QD800 (10 nmol) and DSPE-PEG2000 amine (10 µmol) in chloroform (0.2 mL) were mixed, and the solvent was completely evaporated in a fume hood at room temperature. The residue was re-dissolved in water and sonicated. QD800-PEG nanoparticles (18 nm in diameter) were purified with ultra-centrifugation. For conjugation with Affibody, QD800-PEG (1 nmol) was first activated with the biofunctional linker 4-maleimidobutyric acid N-succinimidyl ester (1 µmol) in borate buffer (pH 8.5) for 2 h at room temperature. After column purification, Cys-Z_HER2:342_ (100 nmol) was incubated with the activated QD800-PEG for 20 min at room temperature with a conjugation efficiency of 40%–50%. QD800-PEG-Z_HER2:342_ nanoparticles were purified with column chromatography. There were ~12 Affibody molecules per nanoparticle with a hydrodynamic diameter of 19 nm.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20in%20vitro)]

Lee et al. (36) performed binding experiments with Cys-Z_HER2:342_ using a Biacore sensor chip immobilized with extracellular domain of chimeric HER2/Fc fusion protein. The dissociation constants (K_d_) of Z_HER2:342_ were calculated to be 30 pM for chimeric HER2/Fc fusion protein. Cellular accumulation studies of QD800-PEG-Z_HER2:342_ were not performed.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20rodentia)]

Gao et al. (35) monitored in vivo biodistribution using NIR optical imaging of HER2-expressing SKOV3 (high HER2 expression) or PC-3 (low HER2 expression) prostate tumors in nude mice (n = 3/group) after intravenous injection of 0.2 nmol QD800-PEG-Z_HER2:342_. Tumor fluorescence intensities were measured at 0.5, 1, 4, 6, and 24 h after tracer injection. QD800-PEG-Z_HER2:342_ showed high fluorescence intensities around the SKOV3 tumor, liver, and kidneys at 4 h after injection. Fluorescence signals in the tumor area peaked at 4 h and decreased gradually but still exhibited good contrast at 24 h. The tumor/background ratios were 2.09 ± 0.11, 2.67 ± 0.29, 3.93 ± 0.54, 2.89 ± 0.16, and 1.87 ± 0.17 at 0.5, 1, 4, 6, and 24 h, respectively. On the other hand, QD800-PEG exhibited tumor/background ratios of 0.84–1.12 at these time points. QD800-PEG-Z_HER2:342_ showed little accumulation in PC-3 tumor with tumor/background ratios of 0.94–1.17 at these time points. No blocking studies were performed.

Ex vivo NIR fluorescence imaging studies were performed at 4 h after injection, with region-of-interest (ROI) analysis of each excised organ (35). The ROI analysis showed high tumor accumulation of 14.9 ± 0.8% injected dose per gram (ID/g) in the mice bearing SKOV3 tumors and injected with QD800-PEG-Z_HER2:342_. SKOV3 tumor accumulation of QD800-PEG and PC-3 tumor accumulation of QD800-PEG-Z_HER2:342_ were 4.3 ± 0.6% ID/g and 5.7 ± 1.8% ID/g, respectively. The organ with the highest concentration was the liver (45% ID/g), followed by the kidney (15% ID/g), spleen (8% ID/g), lung (3% ID/g), intestines (3% ID/g), and muscle (1% ID/g). Histoimmunostaining showed the presence of QD800 fluorescence signal colocalized with tumor cells in the SKOV3 tumor sections from mice injected with QD800-PEG-Z_HER2:342_, but not in SKOV3 tumor sections from mice injected with QD800-PEG or in PC-3 tumor sections from mice injected with QD800-PEG-Z_HER2:342_. QD800-PEG-Z_HER2:342_ nanoparticles are able to extravasate from the CD31-positive tumor vessels and bind to HER2-expressing tumor cells. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20nanoprobes%20and%20human)]

No publication is currently available.

## NIH support

R21 CA121842, U54 CA119367

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Zheng G., Li H., Yang K., Blessington D., Licha K., Lund-Katz S., Chance B., Glickson J.D. (2002). Tricarbocyanine cholesteryl laurates labeled LDL: new near infrared fluorescent probes (NIRFs) for monitoring tumors and gene therapy of familial hypercholesterolemia. Bioorg Med Chem Lett.
12 Gao X., Nie S. (2005). Quantum dot-encoded beads. Methods Mol Biol.
13 Michalet X., Pinaud F.F., Bentolila L.A., Tsay J.M., Doose S., Li J.J., Sundaresan G., Wu A.M., Gambhir S.S., Weiss S. (2005). Quantum dots for live cells, in vivo imaging, and diagnostics. Science.
14 Alivisatos A.P., Gu W., Larabell C. (2005). Quantum dots as cellular probes. Annu Rev Biomed Eng.
15 Hilger I., Leistner Y., Berndt A., Fritsche C., Haas K.M., Kosmehl H., Kaiser W.A. (2004). Near-infrared fluorescence imaging of HER-2 protein over-expression in tumour cells. Eur Radiol.
16 Medintz I.L., Uyeda H.T., Goldman E.R., Mattoussi H. (2005). Quantum dot bioconjugates for imaging, labelling and sensing. Nat Mater.
17 Smith A.M., Gao X., Nie S. (2004). Quantum dot nanocrystals for in vivo molecular and cellular imaging. Photochem Photobiol.
18 Akerman M.E., Chan W.C., Laakkonen P., Bhatia S.N., Ruoslahti E. (2002). Nanocrystal targeting in vivo. Proc Natl Acad Sci U S A.
19 Braydich-Stolle L., Hussain S., Schlager J.J., Hofmann M.C. (2005). In vitro cytotoxicity of nanoparticles in mammalian germline stem cells. Toxicol Sci.
20 Kim S., Lim Y.T., Soltesz E.G., De Grand A.M., Lee J., Nakayama A., Parker J.A., Mihaljevic T., Laurence R.G., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V. (2004). Near-infrared fluorescent type II quantum dots for sentinel lymph node mapping. Nat Biotechnol.
21 Gao X., Cui Y., Levenson R.M., Chung L.W., Nie S. (2004). In vivo cancer targeting and imaging with semiconductor quantum dots. Nat Biotechnol.
22 Han M., Gao X., Su J.Z., Nie S. (2001). Quantum-dot-tagged microbeads for multiplexed optical coding of biomolecules. Nat Biotechnol.
23 Lovric J., Bazzi H.S., Cuie Y., Fortin G.R., Winnik F.M., Maysinger D. (2005). Differences in subcellular distribution and toxicity of green and red emitting CdTe quantum dots. J Mol Med.
24 Ohnishi S., Lomnes S.J., Laurence R.G., Gogbashian A., Mariani G., Frangioni J.V. (2005). Organic alternatives to quantum dots for intraoperative near-infrared fluorescent sentinel lymph node mapping. Mol Imaging.
25 Shiohara A., Hoshino A., Hanaki K., Suzuki K., Yamamoto K. (2004). On the cyto-toxicity caused by quantum dots. Microbiol Immunol.
26 Soltesz E.G., Kim S., Laurence R.G., DeGrand A.M., Parungo C.P., Dor D.M., Cohn L.H., Bawendi M.G., Frangioni J.V., Mihaljevic T. (2005). Intraoperative sentinel lymph node mapping of the lung using near-infrared fluorescent quantum dots. Ann Thorac Surg.
27 Xie R., Chen K., Chen X., Peng X. (2008). InAs/InP/ZnSe Core/Shell/Shell Quantum Dots as Near-Infrared Emitters: Bright, Narrow-Band, Non-Cadmium Containing, and Biocompatible. Nano Res.
28 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
29 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
30 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
31 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
32 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
33 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
34 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
35 Gao J., Chen K., Miao Z., Ren G., Chen X., Gambhir S.S., Cheng Z. (2011). Affibody-based nanoprobes for HER2-expressing cell and tumor imaging. Biomaterials.
36 Lee S.B., Hassan M., Fisher R., Chertov O., Chernomordik V., Kramer-Marek G., Gandjbakhche A., Capala J. (2008). Affibody molecules for in vivo characterization of HER2-positive tumors by near-infrared imaging. Clin Cancer Res.